# Cy5.5-labeled pH low insertion peptide (pHLIP)

Chemical name: | ACEQNPIYWARYADWLFTTPLLLLDLALLVDADEGTG-Cy5.5
Abbreviated name: | pHLIP-Cy5.5
Synonym:
Agent Category: | Peptide
Target: | Low pH
Target Category: | Others
Method of detection: | Near-infrared fluorescence optical imaging
Source of signal / contrast: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | No structure available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?cmd=PureSearch&db=pubmed&term=pHLIP)]

The pH low insertion peptide (pHLIP) is a peptide of 37 amino acids that inserts across the cell membrane as an α-helix when the extracellular pH (pH_e_) is acidic (1-4). pHLIP labeled with the near-infrared (NIR) fluorescent marker Cy5.5 (pHLIP-Cy5.5) was developed by Andreev et al. for optical mapping of areas (tumor and arthritis) of elevated acidity in the small animals (1).

Tumor microenvironment is characterized by low pH_e_ (5, 6). Almost all solid tumors have a neutral to alkaline intracellular pH (pH_i_), but they develop an acidic pH_e_ (known as the Warburg effect, Nobel Prize in 1931 (http://nobelprize.org/nobel_prizes/medicine/laureates/1931/)). The average pH_e_ could be as low as 6.0 (7-9). A pH gradient (pH_i_ > pH_e_) exists across the cell membrane in tumors. This gradient is contrary to that found in normal tissues, in which pH_i_ is lower than pH_e_ (7.2–7.4) (7-9). Diffusion of the H^+^ ions along concentration gradients from tumors into adjacent normal tissues creates a peritumoral acid gradient (10). The mechanisms responsible for the low pH_e_ include anaerobic glycolysis because of hypoxia, aerobic glycolysis (the Warburg effect), increased metabolic CO_2_ production associated with uncontrolled cell growth, and increased activity of ion pumps on the cell membrane (5, 7).

Low pH_e_ affects many aspects of tumor physiology. It is one of the driving forces in the clonal selection leading to invasive and metastatic diseases (11, 12). Rofstad et al. have shown that lowering culture pH to 6.8 results in a promotion of in vivo metastasis of treated human melanoma cells compared with controls (cultured at pH 7.4) after tail vein injection of the cells in mice (13). Exposure of tumor cells to an acidic environment leads to increased expression of various factors that contribute to tumor progression (12). Tumor cells are able to maintain a high proliferation rate in the acidic environment, whereas the peritumoral acid gradient limits immune response to tumor antigens and induces normal cell apoptosis, extracellular matrix degradation, and angiogenesis (7, 11). The passage of noncarrier-mediated weak drugs through the cell membranes is also influenced by the acidic pH_e_ (14-16). Typically, the drugs in an uncharged state (lipophilic form) pass more efficiently through the cell membranes. This leads to the hypothesis of ‘ion-trapping’ that weakly basic drugs will concentrate in more acidic compartments (14, 15). The acid pH_e_ of tumors will therefore hinder weakly basic drugs from reaching their intracellular targets, thereby reducing cytotoxicity (16). Conversely, the acid pH_e_ of tumors will improve uptake of weak acids into the relatively neutral intracellular space (17). The currently used chemotherapeutic drugs such as mitoxantrone, doxorubicin, daunorubicin, anthracyclines, anthraquinones and vinca alkaloids are all weak bases (pKa 5.5–6.8), while cyclophosphamide, 5-fluorouracil and chlorambucil are weak acids (pKa 7.8–8.8) (15). Both in vitro and in vivo studies have shown that the activities of those weak bases are inhibited by the low pH_e_ (14-16). On the contrary, the actions of the weak acids are enhanced by the low pH_e_. The pH gradient in tumors exerts a protective effect upon the cells from weak-base drugs as well as acts to potentiate the action of weak acid drugs (17). Studies have consistently shown that selective tumor alkalinization in vivo is likely to result in an enhancement in the anti-tumor activity of weakly basic chemotherapeutic drugs (18, 19). Low pH_e_ has also been shown to impair the effectiveness of some drugs such as paclitaxel in that their chemical structures do not predict pH-dependent ionization (7). In addition, radiation therapies are known to be significantly less effective at the hypoxic and acidic regions of tumor (20).

An understanding of the mechanisms involved in tumor-specific low pH_e_ leads to the development of targeted therapeutic approaches (6, 7). Low pH_e_ is also considered a promising marker for tumor targeting detection (4, 8). The pHLIP interacts with the surface of membranes as an unstructured peptide at neutral pH_e_, but at acidic pH_e_ (<7.0) it inserts across the membrane and forms a stable transmembrane α-helix (1, 2, 21, 22). The pHLIP affinity for membranes at low pH (5.0) is 20 times higher than that at high pH (8.0). Studies by Zoonens et al. showed that the pHLIP could translocate cell-impermeable cargo molecules across a cell membrane and release them in the cytoplasm (23). The process is mediated by the formation of a transmembrane α-helix because of increased peptide hydrophobicity associated with the protonation of Asp residues at low pH (1, 22). Replacement of the two key Asp residues located in the transmembrane part of pHLIP with Lys or Asn leads to the loss of pH-sensitive membrane insertion (3). Andreev et al. labeled the pHLIP with Cy5.5 and tested its feasibility for optical mapping of tumor and arthritis which were characterized by elevated acidity (1).

Optical fluorescence imaging is increasingly being used to monitor biological functions of specific targets in small animals (24-26). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light are used. Near-infrared (NIR) fluorescence detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a non-invasive alternative to radionuclide imaging in small animals (27, 28).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pHLIP)]

Four peptides (L-pHLIP, D-pHLIP, N-pHLIP, and K-pHLIP) were designed by Andreev et al. (1). L-pHLIP and D-pHLIP were synthesized with the same sequence but from L- and D-amino acids, respectively. The pHLIP peptide sequence was ACEQNPIYWARYADWLFTTPLLLLDLALLVDADEGTG. N-pHLIP and K-pHLIP were used as controls. In N-pHLIP and K-pHLIP, Asn and Lys replaced Asp residues, which are protonated at low pH and drives pHLIP insertion into membrane. All peptides were prepared with solid-phase peptide synthesis using standard 9-fluorenylmethyloxycarbonyl chemistry and purified with reverse-phase chromatography. NIR fluorescent dye Cy5.5 was conjugated with Cys or Lys residues placed on the pHLIP N terminus, which remains outside the cell when the peptide inserts across the lipid bilayer. The detailed purity and degree of labeling of the pHLIP-Cy5.5 conjugate were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pHLIP)]

Andreev et al. analyzed the molecular mechanism of pHLIP insertion in vitro using liposomes and human red blood cells (RBCs) (1). In the presence of liposomes, pHLIP inserted into the lipid bilayer with perpendicular orientation and formed transmembrane α-helix at low pH (4.5) (1, 29). The control K-pHLIP did not show secondary structure changes and remained outside the membrane at pH 4.5 and pH 8.0. N-pHLIP formed an α-helical structure and was found primarily in the membrane over a wide pH range (4.0–8.0). With concentrations up to 10 µM, pHLIP did not cause lysis of the human RBCs at pH 6.0 or pH 7.4 after incubation with RBCs for 1 h at room temperature. Morphologically, incubation of the RBCs (1% suspension) with pHLIP (5 μM) for 15 min resulted in the appearance of spicules on the surface of 67% of the cells at normal pH (7.4), but only on 13% of the cells at low pH (6.0). K-pHLIP (5 μM) induced formation of echinocytes at both pH levels (57% of cells at pH 7.4 and 55% of cells at pH 6.0), and N-pHLIP (5 μM) did not induce shape changes in RBCs (74% and 83% of the cells were discocytes at the respective pH levels). The results indicate that pHLIP inserts into the membrane at low pH (6.0), whereas K-pHLIP weakly binds to the membrane surface and N-pHLIP interacts with lipid vesicles and forms α-helical structure at both pH levels.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pHLIP)]

Andreev et al. tested the ability of pHLIP-Cy5.5 to accumulate in tumors with low pH_e_ and inflammatory arthritis as another model of low pH (1). Mouse tumors were established with subcutaneous injection of murine breast adenocarcinoma cells (CRL-2116) in the right flank of female C3D2F1 mice (number of animals not reported). pHLIP-Cy5.5 (500 µg/kg) was given as a single intraperitoneal injection into the left side of the mice. Optical imaging showed that pHLIP-Cy5.5 was redistributed and concentrated in tumors within 20 h after injection. pHLIP-Cy5.5 was able to mark tumors of various sizes with high accuracy. The fluorescent signal in tumors was stable for 4 days and was ~5 times higher than in the healthy counterpart tissue (n > 20 animals). No specific accumulations were observed in tumors for Cy5.5 dye alone, K-pHLIP-Cy5.5, and N-pHLIP-Cy5.5. Arthritis was induced in the right knee joints with the use of methylated bovine serum albumin and Freund's complete adjuvant. After intraperitoneal injection of pHLIP-Cy5.5 (30 µg/kg), pHLIP-Cy5.5 targeted the inflammatory site in the right leg with no accumulation in the left (control) leg. The fluorescent signal was 4–5 times higher in the right than in the left knee joints.

No significant difference was observed between the accumulation of L-pHLIP-Cy5.5 and D-pHLIP-Cy5.5 in tumor, inflammatory foci, and kidney, indicating that the peptide insertion process does not depend on amino acid chirality. Buffering the feed water to pH 8.2 resulted in ~50% reduction of the fluorescent signal in the kidneys of mice (number of animals not reported) There was no significant accumulation in the liver or other organs. A preliminary toxicity study showed no physiological or behavioral changes within 2 months after intravenous injection of L-pHLIP and D-pHLIP (4 mg/kg) in 4-week-old female and male mice (number of animals not reported).

Andreev et al. concluded that pHLIP nanotechnology offers an approach for mapping areas of elevated acidity in the body, possibly enabling the study of pathological processes, diagnosis of diseases, treatment by delivery of molecules to affected areas, and monitoring of therapeutic outcomes. The authors have reported similar results by labeling pHLIP with NIR dye Alexa750 (detailed data not shown) (1). Vāvere et al. labeled the same peptide with ^64^Cu (^64^Cu-DOTA-pHLIP (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)) and used it for positron emission tomography imaging of low pH_e_ in prostate tumor xenografts (4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pHLIP+pH+imaging)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pHLIP+pH+imaging)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pHLIP+pH+imaging)]

No references are currently available.

## NIH Support

P20RR016457, GM070895, GM073857

## References

1 Andreev O.A., Dupuy A.D., Segala M., Sandugu S., Serra D.A., Chichester C.O., Engelman D.M., Reshetnyak Y.K. (2007). Mechanism and uses of a membrane peptide that targets tumors and other acidic tissues in vivo. Proc Natl Acad Sci U S A.
2 Reshetnyak Y.K., Andreev O.A., Lehnert U., Engelman D.M. (2006). Translocation of molecules into cells by pH-dependent insertion of a transmembrane helix. Proc Natl Acad Sci U S A.
3 Reshetnyak Y.K., Segala M., Andreev O.A., Engelman D.M. (2007). A monomeric membrane peptide that lives in three worlds: in solution, attached to, and inserted across lipid bilayers. Biophys J.
4 Vavere A.L., Biddlecombe G.B., Spees W.M., Garbow J.R., Wijesinghe D., Andreev O.A., Engelman D.M., Reshetnyak Y.K., Lewis J.S. (2009). A novel technology for the imaging of acidic prostate tumors by positron emission tomography. Cancer Res.
5 Fukumura D., Jain R.K. (2007). Tumor microenvironment abnormalities: causes, consequences, and strategies to normalize. J Cell Biochem.
6 Izumi H., Torigoe T., Ishiguchi H., Uramoto H., Yoshida Y., Tanabe M., Ise T., Murakami T., Yoshida T., Nomoto M., Kohno K. (2003). Cellular pH regulators: potentially promising molecular targets for cancer chemotherapy. Cancer Treat Rev.
7 Cairns R., Papandreou I., Denko N. (2006). Overcoming physiologic barriers to cancer treatment by molecularly targeting the tumor microenvironment. Mol Cancer Res.
8 Pathak A.P., Gimi B., Glunde K., Ackerstaff E., Artemov D., Bhujwalla Z.M. (2004). Molecular and functional imaging of cancer: advances in MRI and MRS. Methods Enzymol.
9 Penet M.F., Glunde K., Jacobs M.A., Pathak A.P., Bhujwalla Z.M. (2008). Molecular and functional MRI of the tumor microenvironment. J Nucl Med.
10 Gatenby R.A., Gawlinski E.T., Gmitro A.F., Kaylor B., Gillies R.J. (2006). Acid-mediated tumor invasion: a multidisciplinary study. Cancer Res.
11 Lunt S.J., Chaudary N., Hill R.P. (2009). The tumor microenvironment and metastatic disease. Clin Exp Metastasis.
12 Joyce J.A., Pollard J.W. (2009). Microenvironmental regulation of metastasis. Nat Rev Cancer.
13 Rofstad E.K., Mathiesen B., Kindem K., Galappathi K. (2006). Acidic extracellular pH promotes experimental metastasis of human melanoma cells in athymic nude mice. Cancer Res.
14 Raghunand N., Mahoney B.P., Gillies R.J. (2003). Tumor acidity, ion trapping and chemotherapeutics. II. pH-dependent partition coefficients predict importance of ion trapping on pharmacokinetics of weakly basic chemotherapeutic agents. Biochem Pharmacol.
15 Mahoney B.P., Raghunand N., Baggett B., Gillies R.J. (2003). Tumor acidity, ion trapping and chemotherapeutics. I. Acid pH affects the distribution of chemotherapeutic agents in vitro. Biochem Pharmacol.
16 Gerweck L.E., Kozin S.V., Stocks S.J. (1999). The pH partition theory predicts the accumulation and toxicity of doxorubicin in normal and low-pH-adapted cells. Br J Cancer.
17 Kozin S.V., Shkarin P., Gerweck L.E. (2001). The cell transmembrane pH gradient in tumors enhances cytotoxicity of specific weak acid chemotherapeutics. Cancer Res.
18 Silva A.S., Yunes J.A., Gillies R.J., Gatenby R.A. (2009). The potential role of systemic buffers in reducing intratumoral extracellular pH and acid-mediated invasion. Cancer Res.
19 Swietach P., Vaughan-Jones R.D., Harris A.L. (2007). Regulation of tumor pH and the role of carbonic anhydrase 9. Cancer Metastasis Rev.
20 Vaupel P. (2004). Tumor microenvironmental physiology and its implications for radiation oncology. Semin Radiat Oncol.
21 Tang J., Gai F. (2008). Dissecting the membrane binding and insertion kinetics of a pHLIP peptide. Biochemistry.
22 Reshetnyak Y.K., Andreev O.A., Segala M., Markin V.S., Engelman D.M. (2008). Energetics of peptide (pHLIP) binding to and folding across a lipid bilayer membrane. Proc Natl Acad Sci U S A.
23 Zoonens M., Reshetnyak Y.K., Engelman D.M. (2008). Bilayer interactions of pHLIP, a peptide that can deliver drugs and target tumors. Biophys J.
24 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
25 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
26 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
27 Robeson W., Dhawan V., Belakhlef A., Ma Y., Pillai V., Chaly T., Margouleff C., Bjelke D., Eidelberg D. (2003). Dosimetry of the dopamine transporter radioligand 18F-FPCIT in human subjects. J Nucl Med.
28 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
29 Hunt J.F., Rath P., Rothschild K.J., Engelman D.M. (1997). Spontaneous, pH-dependent membrane insertion of a transbilayer alpha-helix. Biochemistry.